# ^99m^Tc-Labeled citric acid-folate conjugate

Chemical name: | ^99m^Tc-Labeled citric acid-folate conjugate
Abbreviated name: | ^99m^Tc-Citro-folate
Synonym:
Agent Category: | Compounds
Target: | Folate receptor
Target Category: | Receptor
Method of detection: | Single-photon emission computed tomography (SPECT); gamma planar imaging
Source of signal / contrast: | ^99m^Tc
Activation: | No
Studies: | - In Vitro; - Rodents | No structure is available.

## Background

[PubMed]

^99m^Tc-Labeled citric acid-folate conjugate, abbreviated as ^99m^Tc-citro-folate, was synthesized by Altiparmak et al. for folate receptor (FR)-targeted imaging of FR-positive tumors (1).

Folate (folic acid) is an essential vitamin for cell synthesis of nucleotide bases. Some unique features of the FR-folate system make it a valuable target for developing FR-targeted imaging and therapeutic agents (2-4). First, FR has a high affinity for the exogenous folate conjugates (K_d_ = ~100 pM), but the reduced folate carrier and the proton coupled folate transporters display very low or no affinity for folate conjugates. Second, the FR-α isoform is overexpressed in ~40% of human cancer tissues, where it is completely accessible to folate conjugates, but the FR-α is inaccessible for the conjugates in most normal tissues because its expression occurs largely at the apical (luminal) surface of epithelial cells where it is not supplied with blood vessels . Third, folate conjugates are taken up by cancer cells via FR-mediated endocytosis, and FR recycles actively to the cell surface with a frequency of 5.7–20 h, depending on cell types. Fourth, conjugation of imaging labels via the γ-carboxyl group of folate has no apparent effects on the ligand-binding affinity to FR. Furthermore, folate is a small molecule (MW = ~441) and exhibits rapid and complete penetration of solid tumors and rapid clearance from FR-negative tissues (t_1/2_, <10 min). One disadvantage of the FR-folate system is that FR expresses at a relatively low density on the tumor cell surface (1–3 million FR/cell), and binding saturation can be reached rapidly; these characteristics can limit the FR-targeted imaging contrast (5, 6). Therefore, sensitive imaging techniques such as positron emission tomography and single-photon emission computed tomography (SPECT) appear to be more suitable for FR-targeted imaging (2, 3, 7).

To date, a large set of folate-based radiopharmaceutical agents have been synthesized for nuclear imaging. In general, a chelating agent is necessary for bridging the radiolabels and the folate molecule; a chelating agent is also critical for optimizing the pharmacokinetics of the compound (1, 8). Altiparmak et al. synthesized ^99m^Tc-citro-folate using citric acid as a chelating agent (1). Biodistribution studies showed accumulation of the compound in FR-rich tissues and demonstrated its potential for clinical imaging of FR-positive tumors. ^99m^Tc is widely used for nuclear imaging because of its ideal energy (Eγ = 140 keV), low radiation dose, long half-life (t_1/2_, 6 h), and commercial availability (1).

### Related Resource Links:

- FR-targeted chapters (http://www.ncbi.nlm.nih.gov/books/?term=folate%20receptor%20AND%20micad%5bbook%5d) on MICAD
- Protein (http://www.ncbi.nlm.nih.gov/protein/?term=Folate+Receptor) and nucleotide (http://www.ncbi.nlm.nih.gov/nucleotide/?term=Folate+Receptor) information of FR
- FR-targeted clinical trials (http://clinicaltrials.gov/ct2/results?term=Folate+Receptor) in Clinicaltrials.gov

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20696224)]

Altiparmak et al. described the details of ^99m^Tc-citro-folate synthesis (1). The synthesis included three steps. Folate-hydrazide was first synthesized; then it was sequentially conjugated with citric acid to generate citro-folate. The intermediate products, N-hydroxysuccinimide-folate, folate-hydrazide, and citro-folate, were well characterized with different techniques. ^99m^Tc was then labeled to the citric group to produce the desired compound, ^99m^Tc-citro-folate. The radiolabeling efficiency of the final product, ^99m^Tc-citro-folate, was 97 ± 1.0%. The specific radioactivity was 1.32 MBq/mmol (35.68 µCi/mmol).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20696224)]

Stability studies showed that ~95.4% of the ^99m^Tc-citro-folate was intact after 180 min incubation with human serum. The ^99m^Tc-citro-folate was negatively charged and had a low lipophilicity (logD value = −0.96 ± 0.39) (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=20696224)]

Biodistribution of ^99m^Tc-citro-folate in organs with saturated and unsaturated FR was investigated in 18 female Albino Wistar rats at three different time points (60, 120, and 180 min) after intraperitoneal administration of 20 µg (0.03 µmol) ^99m^Tc-citro-folate (n = 3 mice/group) (1). The uptake in organs was expressed as the percent of radioactivity per gram of tissue (% ID/g).

The FR-unsaturated studies (no blocking) showed that the uptake (% ID/g) of ^99m^Tc-citro-folate in small intestine (0.10), large intestine (0.7), stomach (0.07), uterus (0.14), and ovary (0.07) reached the maximum at 60 min after administration of the compound. The uptake at 180 min decreased markedly (P < 0.05) in the large intestine (0.06% ID/g) and stomach (0.02% ID/g). In the FR-rich organs (ovary, uterus, and kidney), the clearance of ^99m^Tc-citro-folate was generally slower than in other organs. The uptake values in the ovary, uterus, and kidneys were 0.04, 0.02, and >0.1% ID/g at 180 min, respectively.

For the FR-saturated studies, each animal was pretreated with 300 µg folic acid through the intraperitoneal route 30 min before injection of ^99m^Tc-citro-folate. Similar to the findings in the unsaturated studies, the ^99m^Tc-citro-folate uptake (% ID/g) reached a maximum at 60 min in the small intestine (0.09), large intestine (0.06), stomach (0.09), kidney (0.06), ovary (0.06), and uterus (0.07). However, the corresponding uptake values (% ID/g) in these organs at 180 min were all lower: 0.04, 0.05, 0.03, 0.10, 0.02, and 0.02, respectively.

Comparison between FR-unsaturated and FR-saturated studies revealed that the uptake in the ovary and uterus decreased when the receptor was saturated (1). The decrease for the ovary was 11%, 41%, and 41% at 60, 120, and 180 min, respectively. The decrease for the uterus was 47%, 31%, and 26% at 60, 120, and 180 min, respectively. Non-radiolabeled folic acid reduced the uptake in FR-rich tissues. The uptake in kidneys increased over time in both studies, suggesting rapid clearance from blood. Hydrophilic conjugates, including ^99m^Tc-citro-folate, generally remain longer in blood because of their negative charge (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are currently available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are currently available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are currently available.

## References

1 Altiparmak B., Lambrecht F.Y., Bayrak E., Durkan K. (2010). Design and synthesis of 99mTc-citro-folate for use as a tumor-targeted radiopharmaceutical. Int J Pharm.
2 Sega E.I., Low P.S. (2008). Tumor detection using folate receptor-targeted imaging agents. Cancer Metastasis Rev.
3 Low P.S., Kularatne S.A. (2009). Folate-targeted therapeutic and imaging agents for cancer. Curr Opin Chem Biol.
4 Zhao X., Li H., Lee R.J. (2008). Targeted drug delivery via folate receptors. Expert Opin Drug Deliv.
5 Konda S.D., Aref M., Wang S., Brechbiel M., Wiener E.C. (2001). Specific targeting of folate-dendrimer MRI contrast agents to the high affinity folate receptor expressed in ovarian tumor xenografts. MAGMA.
6 Low P.S., Henne W.A., Doorneweerd D.D. (2008). Discovery and development of folic-acid-based receptor targeting for imaging and therapy of cancer and inflammatory diseases. Acc Chem Res.
7 Miotti S., Bagnoli M., Ottone F., Tomassetti A., Colnaghi M.I., Canevari S. (1997). Simultaneous activity of two different mechanisms of folate transport in ovarian carcinoma cell lines. J Cell Biochem.
8 Zhang Y., Sun Y., Xu X., Zhu H., Huang L., Zhang X., Qi Y., Shen Y.M. (2010). Radiosynthesis and micro-SPECT imaging of 99mTc-dendrimer poly(amido)-amine folic acid conjugate. Bioorg Med Chem Lett.